# AOI987

Chemical name: | AOI987
Abbreviated name: | AOI987
Synonym:
Agent Category: | Compound
Target: | Aggregates of β-amyloid (Aβ) peptides
Target Category: | Acceptor
Method of detection: | Optical imaging (NIRF)
Source of signal: | AOI987
Activation: | No
Studies : | - In vitro; - Rodent | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AOI987%5BAll%20Fields%5D)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?CMD=search&DB=pubmed]

Alzheimer’s disease (AD) is a major neurodegenerative disease associated with an irreversible decline of mental functions and with cognitive impairment (1, 2). It is characterized by the presence, in the brain, of senile plaques of β-amyloid (Aβ) peptides with intracellular neurofibrillary tangles of filaments containing the hyperphosphorylated protein tau (3, 4). Accelerated deposition of Aβ deposits seems to be a key risk factor associated with AD, and although the mechanisms of the disease are still not fully understood, reducing the deposition of amyloid plaques seems to benefit patients.

Today, the clinical diagnosis of AD relies on mental and cognitive assessments of patients and the confirmation of the disease is so far obtained by postmortem examination of tissues. Major effort is being undertaken to find means of evaluating in vivo, at an early stage, the growth of the Aβ plaques for better assessment and possibly treatment.

Several radioligands for positron emission tomography (PET), such as [^18^F]FDDNP (5), with [^11^C]PIB (6), and [^11^C]SB-13, have been developed and tested in humans in vivo (7-9). Although PET currently seems to be the most promising technique, it has several drawbacks, including the short half-lives of the positron emitting nuclei and the limited availability of the technique. Magnetic resonance imaging (MRI) does have somewhat stringent requirements on spatial resolution in order to identify individual plaques (diameter ≤ 50 µm), and while feasible on fixed human specimen using transgenic mouse models, the clinical use has not been yet possible.

Recent studies have been carried out using an alternative, all-optical, imaging technology that uses novel fluorescent amyloid dyes that absorb and emit in the near-infrared (NIR) spectrum (10-13). NIR imaging reduces the background and scattering through biological tissue usually encountered with fluorescent imaging in live animals with short wavelengths of light; it has been shown as a viable alternative for visualizing amyloid load in living mice using a fluorescent dye such as AOI987 (13). AOI987 possesses all the main characteristics needed to image Aβ plaques: 1) a low molecular weight (< 500 Da), 2) a high lipophilicity (logP 1-4, P = partition coefficient) to cross the blood-brain barrier (BBB) in sufficient amounts, 3) a fluorescence maximum within 650-900 nm.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AOI987%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D]

AOI987 can be prepared following a two-step procedure using an azo derivative as key intermediate, as described by Hintersteiner et al. (13). In this procedure, the authors prepared the azo intermediate (4-methyl-7-(4-nitro-phenylazo)-3,4-dihydro-2H-benzo[1,4]oxazin-6-ol) by dissolving 4-nitro-benzenediazonium tetrafluoroborate in 10% H_2_SO_4_, and subsequently adding the obtained solution to 4-methyl-3,4-dihydro-2H-benzo[1,4]oxazine-6-ol in methanol. After stirring for 30 min at 20 °C, the mixture was then neutralized with 25% aqueous ammonia, and a red precipitate containing the azo intermediate was spun down. Purification of the product was made by recrystallization in n-butanol. The chemical purity obtained was > 95%.AOI987 was prepared by dissolving the azo intermediate (560 mg, 1.78 mmol) and 4-methyl-3,4-dihydro-2H-benzo[1,4]oxazin-6-ol (326 mg, 1.96 mmol) into a mixture of ethanol/water (10:1, 10 ml). After an addition of 32% HCl (700 µl), the mixture was then stirred for 1 h at 70 °C (under reflux, and finally, and was finally concentrated under reduced pressure. The obtained residue was dissolved in water and treated with a saturated solution of sodium tetrafluoroborate. The precipitate formed by this reaction was spun down and purified using a column chromatography (SiO_2 >_ dichloromethane/methanol = 10:2) to produce the blue crystals of AOI987 (480 mg (1.17 mmol), 65%).

AOI987 displayed the following fluorescent properties: one single absorption maximum at 650 nm, one single emission maximum at 670 nm, a moderate absorption coefficient of 64,570 M^-1^cm^-1^, and a very high quantum yield (41%, in mouse serum) (13)

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AOI987%20AND%20in%20vitro)]

The binding of AOI987 to amyloid plaques was assessed by incubating brain slices of female APP23 mice (average body weight ~ 25g, 3 ≤ n ≤ 5) for 5 min at 20 °C with aqueous solutions of the dye, at various concentrations ranging from 0.0001% to 0.01% (wt/vol). An analysis of the tissue sections showed that the fluorescent spots co-localized with Aβ deposits stained with silver methenamine, indicating a specific staining of amyloid plaques by the oxazine dye. AOI987 showed an excellent contrast-to-noise ratio, even at very low concentrations (lowest concentration in the study was 0.0001% (wt/vol)) (13)

Differential fluorescence spectroscopy performed by Hintersteiner et al. (13) showed that the magnitude of the fluorescence shift was dependent on the concentration of aggregated Aβ peptides. The K_d_ value for AOI987 was estimated to be 0.2 µM. Additional studies were also performed by the authors using aggregated Aβ peptides incubated with thioflavin T to study related thioflavin T displacement. The measured fluorescence intensity showing a maximum between 460 and 560 nm (excitation 445 nm) reflected thioflavin binding to aggregated Aβ peptides. Addition of AOI987 caused a concentration-dependent reduction of the fluorescence intensity, indicating displacement of thioflavin from aggregated Aβ peptide. A calculation of the apparent binding constant for AOI987 (to aggregated A peptide) was made by measuring displacement curves, leading to values in the range of 0.1 –0.2 µM, for all thioflavin concentrations. The fact that the apparent binding constant did not increase with the thioflavin concentration showed that the displacement of thioflavin from aggregates Aβ did not occur by a simple competitive mechanism.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AOI987%20AND%20rodentia%5BMeSH%5D)]

The BBB penetration of AOI987 was assessed ex-vivo by Hintersteiner et al. (13), using groups of n=4 wild-type mice (C57BL/6Jico). Briefly, the experimental protocol involved injecting the dye intravenously to the animals (injection volume of 10ml/kg of tissue, using 0.9% saline as vehicle). After sacrifice of the mice at various time points (n = 4 each, 5 min to 2 h), AOI987 levels were determined in plasma and brain tissue extracts using liquid chromatography/mass spectrometry methods.

Results showed a maximal plasma concentration of AOI987 obtained within 15 min after injection. The dye was rapidly eliminated from circulation, with residual plasma levels < 10% of the initial concentration, 2 h after administration. The elimination of AOI987 from the brain compartment was slightly slower and the brain concentration of AOI987 was greater than the corresponding plasma levels at all time points measured by the authors, indicating a rapid and significant penetration of AOI987 through the intact blood-brain barrier. In this study (13), the limit of quantification reported was 3 pmol/ml plasma and 15 pmol/g brain.In vivo NIRF imaging of Aβ using AOI987 was also reported by Hintersteiner et al. (13). The experiments were carried out with female 17-month-old APP23 transgenic mice (n = 3 to 5) and age-matched wild-type littermates (n = 2 to 4). AOI987 was injected intravenously through the tail vein at the following concentrations: 0.1 (established optimal dose), 1 and 3 mg/kg of tissue (in 0.9% saline). Results showed an intense fluorescence signal in the brain, very shortly after injection of the dye. The disappearance of the fluorescence signal was substantially slower in transgenic APP23 as compared with wild-type animals. Reported values (extracted from figures provided by the authors) of the relative fluorescence signal (in %), using the optimal dose of injected dye, were as follows: ~62 at 60 min post-injection (no significant difference between wild and APP23 mice); ~40 for wild-type mice and ~50 for APP23 mice, at 120 min post-injection (P < 0.001); ~40 for wild-type mice and ~25 for APP23 mice, at 240 min post-injection.

In their study, Hintersteiner et al. (13) defined ‘specific binding’ of AOI987 as (the fluorescence signal for transgenic mice – the fluorescence signal for wild-type mice)/the flurorescence signal for transgenic mice. The reported values for specific binding (extracted from figures), after injection of 0.1mg/kg AOI987 were as follows: ~0.25 at 60 min post-injection, ~0.4 at 120 min post-injection.

Additional NIRF-AOI987 in vivo studies using younger mice showed a similar signal pattern between 6-month- and 9-month-old mice, and a complementary histological analysis showed that the minimum age at which the differences between AAP23 transgenic and wild-type mice was 9 months.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AOI987%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AOI987%20AND%20%28baboon%20OR%20%28primates%20NOT%20human%29%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AOI987%20AND%20human)]

No publication is currently available.

## References

1 Heininger K. (2000). A unifying hypothesis of Alzheimer's disease. IV. Causation and sequence of events. Rev Neurosci, 11 Spec No: p. 213-328.
2 Forstl H, Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
3 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
4 Brandt R, Leschik J. (2004). Functional interactions of tau and their relevance for Alzheimer's disease. Curr Alzheimer Res.
5 Shoghi-Jadid K, Small GW, Agdeppa ED, Kepe V, Ercoli LM, Siddarth P, Read S, Satyamurthy N, Petric A, Huang SC, Barrio JR. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
6 Klunk WE, Engler H, Nordberg A, Wang Y, Blomqvist G, Holt DP, Bergstrom M, Savitcheva I, Huang GF, Estrada S, Ausen B, Debnath ML, Barletta J, Price JC, Sandell J, Lopresti BJ, Wall A, Koivisto P, Antoni G, Mathis CA, Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
7 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
8 Bacskai BJ, Hickey GA, Skoch J, Kajdasz ST, Wang Y, Huang GF, Mathis CA, Klunk WE, Hyman BT. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
9 Wu C, Pike VW, Wang Y. (2005). Amyloid imaging: from benchtop to bedside. Curr Top Dev Biol.
10 Nesterov EE, Skoch J, Hyman BT, Klunk WE, Bacskai BJ, Swager TM. (2005). In vivo optical imaging of amyloid aggregates in brain: design of fluorescent markers. Angew Chem Int Ed Engl.
11 Skoch J, Dunn A, Hyman BT, Bacskai BJ. (2005). Development of an optical approach for noninvasive imaging of Alzheimer's disease pathology. J Biomed Opt.
12 Frangioni JV. (2006). Self-illuminating quantum dots light the way. Nat Biotechnol.
13 Hintersteiner M, Enz A, Frey P, Jaton AL, Kinzy W, Kneuer R, Neumann U, Rudin M, Staufenbiel M, Stoeckli M, Wiederhold KH, Gremlich HU. (2005). In vivo detection of amyloid-beta deposits by near-infrared imaging using an oxazine-derivative probe. Nat Biotechnol.